# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Asp-Gly-Glu-Ala

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Asp-Gly-Glu-Ala
Abbreviated name: | ^64^Cu-DOTA-DGEA
Synonym:
Agent category: | Peptide
Target: | Integrin α_2_β_1_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAF77577.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_002203.3) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3673) for more information about integrin α_2_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-DGEA)]

Integrins are a family of cell-surface heterodimeric glycoproteins that mediate diverse biological events (e.g., cell adhesion, migration, differentiation, proliferation, and apoptosis) involving cell–cell and cell–matrix interactions (1, 2). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. On the other hand, integrins affect tumor growth, tumor invasiveness, and metastasis (3, 4). The α_2_β_1_ integrin receptor binds mainlycollagen type I, laminins, E-cadherin, and matrix metalloproteinase 1 (5). The α_2_β_1_ integrin is strongly expressed on tumor cells and has been implicated in tumor progression and metastasis (6, 7). In particular, prostate cancer cells and prostate cancer stem cells express high levels of α_2_β_1_ integrin (8, 9). A tetrapeptide sequence consisting of Asp-Gly-Glu-Ala (DGEA) has been identified as a recognition motif used by the type I collagen to bind to α_2_β_1_ integrin (10). DGEA was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in prostate tumor-bearing mice (11). Cy5.5-DGEA has been shown to have a high accumulation in α_2_β_1_-positive PC-3 human prostate tumor cells in nude mice. For positron emission tomography (PET) imaging of α_2_β_1_ integrin, ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-DGEA (^64^Cu-DOTA-DGEA) was prepared and evaluated in nude mice bearing human PC-3 prostate tumors (12).

### Related Resource Links:

- Chapters in MICAD (DGEA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=DGEA+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_2_ integrin (http://www.ncbi.nlm.nih.gov/gene/3673), β_1_ integrin (http://www.ncbi.nlm.nih.gov/gene/3688))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_2_ integrin (http://www.ncbi.nlm.nih.gov/omim/192974), β _1_ integrin (http://www.ncbi.nlm.nih.gov/omim/135630))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-DGEA+synthesis)]

DOTA-DGEA was obtained using solid-phase synthesis (12). The N-hydroxysuccinimide ester of DOTA reacted with the N-terminal amino group of the Asp of the DGEA peptides. The measured mass of DOTA-DGEA peptide conjugates confirmed the 1:1 addition. DOTA-DGEA was incubated with ^64^CuCl_2_ in sodium acetate buffer (pH 5.5) for 60 min at 40°C. ^64^Cu-DOTA-DGEA was purified with high-performance liquid chromatography. This procedure provided a radiolabeling yield of >90%, with a specific activity of 10.7 GBq/µmol (0.29 Ci/µmol) and a radiochemical purity of >98%. ^64^Cu-DOTA-DGEA was 91%, 69%, and 45% intact for 4, 12, and 48 h, respectively, at 40°C in phosphate-buffered saline (PBS). Up to 55% of ^64^Cu^2+^ was released in the PBS from ^64^Cu-DOTA-DGEA at 48 h of incubation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-DGEA+and+in+vitro)]

Flow cytometry analysis showed that 99.7% of PC-3 cells, 51.4% of CWR-22 cells, and 15.6% of LNCaP cells were positive for the α_2_β_1_ receptors using FAM-DGEA (11). Binding of 1 µM FAM-DGEA to the three cell types was analyzed with fluorescence microscopy. PC-3 cells exhibited a higher fluorescence intensity signal than CWR-22 and LNCaP cells. The binding of FAM-DGEA to PC-3 cells was completely blocked with 20 µM DGEA.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-DGEA+rodentia)]

Huang et al. (12) performed PET imaging in nude mice (n = 3) bearing PC-3 tumors at 30 min after injection of 11.1 MBq (0.3 mCi) ^64^Cu-DOTA-DGEA. The tumors were clearly visualized. The tumor accumulation value was 0.92 ± 0.53% injected dose/gram (ID/g). The liver and kidney accumulation values were 5.9 ± 0.4% ID/g and 5.3 ± 0.4% ID/g, respectively. The high kidney and liver accumulation for ^64^Cu-DOTA-DGEA was due to its substantial release of ^64^Cu ions. Therefore, the investigators suggested that ^64^Cu-DOTA-DGEA is not suitable for imaging studies. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-DGEA+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-DGEA+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-DGEA+human)]

No publication is currently available.

## References

1 Hynes R.O. (2009). The extracellular matrix: not just pretty fibrils. Science.
2 Barczyk M., Carracedo S., Gullberg D. (2010). Integrins. Cell Tissue Res.
3 Makrilia N., Kollias A., Manolopoulos L., Syrigos K. (2009). Cell adhesion molecules: role and clinical significance in cancer. Cancer Invest.
4 Brooks S.A., Lomax-Browne H.J., Carter T.M., Kinch C.E., Hall D.M. (2010). Molecular interactions in cancer cell metastasis. Acta Histochem.
5 Heino J. (2000). The collagen receptor integrins have distinct ligand recognition and signaling functions. Matrix Biol.
6 Barbolina M.V., Moss N.M., Westfall S.D., Liu Y., Burkhalter R.J., Marga F., Forgacs G., Hudson L.G., Stack M.S. (2009). Microenvironmental regulation of ovarian cancer metastasis. Cancer Treat Res.
7 Kirkland S.C., Ying H. (2008). Alpha2beta1 integrin regulates lineage commitment in multipotent human colorectal cancer cells. J Biol Chem.
8 Hall C.L., Dai J., van Golen K.L., Keller E.T., Long M.W. (2006). Type I collagen receptor (alpha 2 beta 1) signaling promotes the growth of human prostate cancer cells within the bone. Cancer Res.
9 Kiefer J.A., Farach-Carson M.C. (2001). Type I collagen-mediated proliferation of PC3 prostate carcinoma cell line: implications for enhanced growth in the bone microenvironment. Matrix Biol.
10 Staatz W.D., Fok K.F., Zutter M.M., Adams S.P., Rodriguez B.A., Santoro S.A. (1991). Identification of a tetrapeptide recognition sequence for the alpha 2 beta 1 integrin in collagen. J Biol Chem.
11 Huang C.W., Li Z., Conti P.S. (2011). In Vivo Near-Infrared Fluorescence Imaging of Integrin alpha2beta1 in Prostate Cancer with Cell-Penetrating-Peptide-Conjugated DGEA Probe. J Nucl Med.
12 Huang C.W., Li Z., Cai H., Shahinian T., Conti P.S. (2011). Biological stability evaluation of the alpha2beta1 receptor imaging agents: diamsar and DOTA conjugated DGEA peptide. Bioconjug Chem.